# ^64^Cu-Labeled anti-c-kit monoclonal antibody 12A8 Fab fragment

Chemical name: | ^64^Cu-Labeled anti-c-kit monoclonal antibody 12A8 Fab fragment
Abbreviated name: | [^64^Cu]12A8 Fab
Synonym:
Agent Category: | Antibody fragment
Target: | Proto-oncogene c-Kit; tyrosine-protein kinase kit; mast/stem cell growth factor receptor; CD117
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=c-kit&cmd=DetailsSearch)]

The c-kit (CD 117 antigen or stem cell factor ligand receptor) is a 145-kDa type III glycoprotein receptor tyrosine kinase (TK; encoded by the KIT proto-oncogene) that has a TK at the juxtamembrane position, which is activated when a ligand binds to the extracellular ligand-binding domain of the receptor (1). Almost 70% of gastrointestinal stromal tumors (GISTs) (http://www.cancer.gov/cancertopics/pdq/treatment/gist/HealthProfessional) are known to overexpress a c-kit that has a mutation in exon 11 and produces a constitutively activated TK that promotes the survival and proliferation of cells and leads to the development of a malignant phenotype in the cells of the GISTs (1, 2). The biology and mutations of the c-kit gene and the detection, diagnosis, and chemotherapy of cancerous GISTs are discussed in detail elsewhere (3, 4). An immunohistochemical method is commonly used to detect the overexpression of c-kit in GIST cancers, but this invasive technique is known to generate variable results (3, 5). In addition, investigators often use positron emission tomography (PET) with ^18^F-fluoro-deoxyglucose to detect, monitor, and assess the response of GISTs to chemotherapy with imatinib, but this radiolabeled probe does not distinguish between GISTs and other cancerous tumors that have an epithelial or lymphatic origin (6).

Recently, the ^111^In-labeled anti–c-kit monoclonal antibody (mAb) 12A8 ([^111^In]12A8) was developed and evaluated for the detection of GISTs with single-photon emission computed tomography (SPECT) in nude mice bearing xenograft tumors that express c-kit (6). However, with [^111^In]12A8 the tumors were first visible on the animals at 48 h postinjection (p.i.) and became clearly visible only at 96 h p.i. This indicated that it was necessary to develop a radiolabeled immunoreagent that would have superior pharmacokinetic properties and yield faster results compared to the ^111^In-labeled mAb. It is well known that mAb fragments such as Fab (~50 kDa) and single-chain antibody fragments (~27 kDa) have superior in vivo pharmacokinetic properties compared to intact mAbs (~150 kDa) (7, 8). In an effort to achieve this goal, a Fab fragment of mAb 12A8 was labeled with ^111^In (to obtain [^111^In]12A8 Fab) and with ^64^Cu (to obtain [^64^Cu]12A8 Fab), and the two probes were evaluated for the detection of tumors that express c-kit in nude mice (2). This chapter describes PET studies performed with [^64^Cu]12A8 Fab. The detection of tumors that express c-kit with [^111^In]12A8 Fab is discussed in a separate chapter of MICAD (www.micad.nih.gov) (9).

### Other Sources of Information

c-kit–Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=c-kit+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human c-kit (also known as Hardy-Zuckerman 4 feline sarcoma viral oncogene-like protein (KIT)) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/HM015525.1) sequence (Source: NCBI GenBank)

Gene (http://www.ncbi.nlm.nih.gov/nuccore?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=3815) (human c-kit; Gene ID: 3815)

c-kit in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=c-kit)

Signaling events (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200175&source=NATURE&output-format=graphic&ppage=1&genes_a=3815) mediated by c-kit (Source: Pathways Interaction Database)

c-kit–Related clinical trials (http://clinicaltrials.gov/ct2/results?term=c-kit)

Information on c-kit in PubChem Bioassay (http://www.ncbi.nlm.nih.gov/pcassay/?term=c-kit)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20synthesis&cmd=DetailsSearch)]

The source of the 12A8 Fab fragment, its conjugation with 2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), and labeling with ^64^Cu have been described by Yoshida et al. (2). Using cellulose acetate electrophoresis, the DOTA:Fab ratio of this conjugate was estimated to be 1.1. The radiochemical yield and purity of [^64^Cu]12A8 Fab were reported to be 59.6% and 99.7% (n = 1 experiment), respectively, with a specific activity of 4.5 MBq/μmol (~122 μCi/μmol; n = 1 experiment).

For comparative studies, the 12A8 Fab fragment was also conjugated to N-[(R)-2-amino-3-(p-isothiocyanato-phenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (DTPA) and labeled with ^111^In as described elsewhere (2). The radiochemical yield and purity of [^111^In]12A8 Fab were reported to be 61.7 ± 15.9% and 98.4 ± 1.3%, respectively, with a specific activity of 1.2 ± 0.3 MBq/μmol (~32.4 ± 8.0 μCi/μmol; n = 3 experiments).

For use as a control, the IgG_1_ 12A8 mAb was also conjugated to DTPA and labeled with ^111^In to obtain [^111^In]IgG as described above (2). Using cellulose acetate electrophoresis, the DTPA:mAb ratio of this conjugate was determined to be 1.1. The radiochemical yield and purity of [^111^In]IgG were reported to be 61.7 ± 15.9% and 98.4 ± 1.3%, respectively, with a specific activity of 3.4 ± 0.9 MBq/μmol (91.8 ± 24.3 μCi/μmol; n = 3 experiments).

For in vitro studies, the 12A8 Fab fragment was labeled with ^125^I using the chloramine-T method (2). The radiochemical yield and purity of [^125^I]12A8 Fab were reported to be 84.4% and 98.0%, respectively, with a specific activity of 37.5 MBq/μmol (~1 mCi/μmol; n = 1 experiment).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20in%20vitro&cmd=DetailsSearch)]

The in vitro cell binding characterization was performed only for [^111^In]12A8 IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab using human small cell lung cancer cells (SY cells) that express high levels of c-kit (confirmed with Western blot analysis) (2). The cell binding specificities of [^111^In]IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab were determined to be 50.2%, 37.1%, and 39.2%, respectively. The equilibrium dissociation constants of [^111^In]IgG, [^111^In]12A8 Fab, and [^125^I]12A8 Fab were reported to be 8.0, 18.4, and 18.5 nM, respectively, as determined with a competitive inhibition assay in the presence of increasing concentrations of the unlabeled mAb. The amounts of membrane-bound radioactivity from [^111^In]12A8 Fab and [^125^I]12A8 Fab were observed to decrease with time, but only cells exposed to [^111^In]12A8 Fab showed an increased internalization of the label that reached a maximum of ~15% after incubation for 20 h at 37°C. During the same time, the internalization of [^125^I]12A8 Fab decreased from ~15% at 1 h after incubation to ~8% at 20 h after incubation, and a corresponding increase in the amount of non–protein-bound radioactivity was observed in the growth medium. From this study, the investigators concluded that either free ^125^I or some labeled catabolites of [^125^I]12A8 Fab were released into the cell growth medium during the incubation, which indicated that the radioiodinated mAb fragment was not stable under these study conditions (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^64^Cu]12A8 Fab, [^111^In]12A8 IgG, and [^111^In]12A8 Fab were studied in nude mice bearing SY cell tumors and A4 cell tumors (NIH-3T3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1658&Template=cellBiology) that are transfected with the human epidermal growth factor receptor gene and do not express human c-kit) on the left and right thighs, respectively (2). To determine the amount of radioactivity that accumulated in the blood, tumor, and other major organs of the animals, the mice (n = 5 animals/group) were administered the ^64^Cu- or ^111^In-labeled tracer. Animals administered with [^111^In]IgG were euthanized at 24, 48, and 96 h p.i., and animals administered with [^64^Cu]12A8 Fab or [^111^In]12A8 Fab were euthanized at 1, 6, and 12 h p.i. Data obtained from these studies were standardized to a 20-g body weight mouse and presented as percent of injected dose per gram tissue (% ID/g).

The accumulation values of [^64^Cu]12A8 Fab in the SY tumors were 2.6 ± 0.7% ID/g, 6.1 ± 0.2% ID/g, and 6.2 ± 2.0% ID/g at 1, 6, and 12 h p.i., respectively, compared to values of 3.9 ± 0.5% ID/g, 4.8 ± 0.8% ID/g, and 2.8 ± 0.3% ID/g in the A4 tumors at the same time points (2). The uptake values of radioactivity in the SY tumors at 6 h and 12 h p.i. were significantly higher (P < 0.01) than those observed with [^111^In]12A8 Fab at the same time points (see below for details with [^111^In]12A8 Fab). In addition, the renal uptake of radioactivity from [^64^Cu]12A8 Fab was significantly lower (P < 0.01) than that observed with the ^111^In-labeled mAb fragment. The tumor/blood (T/B) ratios for the SY tumors were 0.2, 1.8, and 3.7 at 1, 6, and 12 h p.i. respectively. The T/B ratio at 12 h p.i. was observed to be higher with [^111^In]12A8 Fab than with [^64^Cu]12A8 Fab.

In another study, serial PET images were acquired from a mouse injected with [^64^Cu]12A8 Fab at 1, 6, and 15 h p.i (2). In these images, the SY tumors were not visible at 1 h p.i., but they were clearly visible at 6 h and 15 h p.i., indicating that the tracer was eliminated from the various organs, including blood, by 6 h p.i. Although the imaging data with [^111^In]12A8 Fab were not presented in the publication, the investigators reported that the PET images obtained with [^64^Cu]12A8 Fab at 6 h and 15 h p.i. were more clear than the SPECT images acquired with either [^111^In]12A8 IgG (6) or [^111^In]12A8 Fab (2).

The radioactivity uptake values for [^111^In]12A8 IgG in the A4 tumors were 6.0 ± 0.6% ID/g, 6.5 ± 0.7% ID/g, and 5.6 ± 0.8% ID/g at 24, 48, and 96 h p.i., respectively, compared to values of 15.5 ± 1.9% ID/g, 23.3 ± 2.3% ID/g, and 20.3 ± 1.6% ID/g for [^111^In]12A8 IgG in the SY tumors at the same time points. The T/B ratio for the SY tumors was 1.0 at 24 h p.i. and increased to 2.8 at 96 h p.i. All other organs showed a low uptake of the label that decreased gradually with time.

With [^111^In]12A8 Fab, the uptake values of the tracer in the A4 tumors were 2.7 ± 0.3% ID/g, 2.1 ± 0.3% ID/g, and 1.3 ± 0.2% ID/g at 1, 6, and 12 h p.i., respectively, compared to 2.7 ± 0.5% ID/g, 4.8 ± 0.8% ID/g, and 4.4 ± 1.2% ID/g at the same time points for the SY tumors. The T/B ratios for the SY tumors were 0.3, 3.3, and 9.7 at 1, 6, and 12 h, respectively. All other organs except the kidneys showed a decrease in radioactivity with time. The accumulation of tracer in the kidneys at 6 h p.i. was observed to be 52.5 ± 5.0% ID/g, and the accumulation decreased to 35.8 ± 4.2% ID/g at 12 h p.i., indicating that the radioactivity was excreted primarily through the renal route.

From these studies, the investigators concluded that both [^64^Cu]12A8 Fab and [^111^In]12A8 Fab were suitable to detect GISTs with PET and SPECT, respectively, in rodents (2). However, PET images generated with [^64^Cu]12A8 Fab were more clear than the SPECT images obtained with either [^111^In]12A8 IgG or [^111^In]12A8 Fab.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5D-12A8%20Fab%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Aubin F., Blanke C.D. (2011). Metastatic gastrointestinal stromal tumors. Cancer Chemother Pharmacol.
2 Yoshida C., Tsuji A.B., Sudo H., Sugyo A., Sogawa C., Inubushi M., Uehara T., Fukumura T., Koizumi M., Arano Y., Saga T. (2011). Development of positron emission tomography probe of 64Cu-labeled anti-C-kit 12A8 Fab to measure protooncogene C-kit expression. Nucl Med Biol.
3 Corless C.L., Heinrich M.C. (2008). Molecular pathobiology of gastrointestinal stromal sarcomas. Annu Rev Pathol.
4 Wang W.L., Conley A., Reynoso D., Nolden L., Lazar A.J., George S., Trent J.C. (2011). Mechanisms of resistance to imatinib and sunitinib in gastrointestinal stromal tumor. Cancer Chemother Pharmacol.
5 Miettinen M., Lasota J. (2005). KIT (CD117): a review on expression in normal and neoplastic tissues, and mutations and their clinicopathologic correlation. Appl Immunohistochem Mol Morphol.
6 Sogawa C., Tsuji A.B., Sudo H., Sugyo A., Yoshida C., Odaka K., Uehara T., Arano Y., Koizumi M., Saga T. (2010). C-kit-targeted imaging of gastrointestinal stromal tumor using radiolabeled anti-c-kit monoclonal antibody in a mouse tumor model. Nucl Med Biol.
7 Accardi L., Di Bonito P. (2010). Antibodies in single-chain format against tumour-associated antigens: present and future applications. Curr Med Chem.
8 Marik J., Junutula J.R. (2011). Emerging role of immunoPET in receptor targeted cancer therapy. Curr Drug Deliv.
9 Chopra, A., 111In-Labeled DTPA conjugated anti-c-kit monoclonal antibody 12A8 Fab fragment. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.